# Gadolinium-G6 dendrimer-Cy5.5

Chemical name: | Gadolinium-G6 dendrimer-Cy5.5
Abbreviated name: | Gd-G6-Cy5.5
Synonym:
Agent category: | Macromolecule, polymer
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI), optical, near-infrared (NIR) fluorescence imaging
Source of signal/contrast: | Cy5.5, gadolinium (Gd)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-G6-Cy5.5)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals.

The sentinel lymph node (SLN) is considered to be the first lymph node to receive lymphatic flow from tumor sites and therefore will contain metastatic tumor cells (4). SLN mapping has been used in the diagnosis of metastasis of solid tumors (5). Radical lymph node dissection is performed in patients with malignant cells in the SLNs. SLN mapping is currently performed by a combination of radioactive tracer and blue dye with low spatial resolution. The current procedure is time-consuming and requires a steep learning curve. NIR quantum dots (QDs) have been studied in SLN mapping in small animals (6, 7). However, there are only limited studies of long-term toxicity of QDs in animals (8). Dendrimer consists of a core with concentric annular shells or generations (G1–G6) made of highly branched polymers, which contain numerous surface functional groups for additional modifications. Koyama et al. (9) prepared a G6 dendrimer tagged with Cy5.5 and gadolinium (Gd) for optical NIR fluorescence and magnetic resonance (MR) multimodal imaging of the SLNs.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-G6-Cy5.5%20and%20synthesis)]

G6 dendrimer (~9 nm in diameter) was conjugated with a two-fold molar excess of the bifunctional chelating agent 1B4M-diethylenetriaminepentaacetic acid (1B4M-DTPA) to form G6-1B4M dendrimer (9, 10). There were 142–191 1B4M-DTPA moieties per G6-1B4M dendrimer. Cy5.5-N-Hydroxysuccinimide ester was reacted with the free primary amines of G6-1B4M to form G6-1B4M-Cy5.5. Finally, G6-1B4M-Cy5.5 was incubated with Gd(OAc)_3_ in 0.3 M citrate buffer (pH 4.5) for 18 h for Gd complexing with the DTPA moieties in G6-1B4M-Cy5.5. Gd-G6-Cy5.5 was purified with dialysis. Gd-G6-Cy5.5 contained ~172 Gd ions and 2 Cy5.5 molecules per G6 dendrimer.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-G6-Cy5.5%20and%20in%20vitro)]

Talanov et al. (10) showed that Gd-G6-Cy5.5 (145 Gd, 1.25 Cy5.5) exhibited T1 and T2 relaxivity values of 13.9 and 36.5 mmol^-1^s^-1^, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-G6-Cy5.5%20and%20rodentia)]

Koyama et al. (9) performed MR imaging (3 T) and NIR optical imaging in female nude mice (n = 10) after injection of Gd-G6-Cy5.5 into the left mammary pad. Thirty lymph nodes were examined in each mouse. For MR lymphography studies, a dose of 750 nmol Gd-G6-Cy5.5 was required to consistently visualize at least one SLN in the axillary region in 20–30 min after injection. On the other hand, only 1.2 nmol of Gd-G6-Cy5.5 was required to visualize the axillary SLNs with NIR imaging. When the skin was incised, all SLNs could be easily identified and distinguished from nearby non-SLNs on the basis of their fluorescence. There was a significant correlation (r = 0.86) of fluorescence signal of resected SLNs with MR lymphography measured in vivo and in vitro.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-G6-Cy5.5%20and%20pig)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-G6-Cy5.5%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-G6-Cy5.5%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Morton D.L., Wen D.R., Wong J.H., Economou J.S., Cagle L.A., Storm F.K., Foshag L.J., Cochran A.J. (1992). Technical details of intraoperative lymphatic mapping for early stage melanoma. Arch Surg.
5 Schulze T., Bembenek A., Schlag P.M. (2004). Sentinel lymph node biopsy progress in surgical treatment of cancer. Langenbecks Arch Surg.
6 Frangioni J.V., Kim S.W., Ohnishi S., Kim S., Bawendi M.G. (2007). Sentinel Lymph Node Mapping With Type-II Quantum Dots. Methods Mol Biol.
7 Zimmer J.P., Kim S.W., Ohnishi S., Tanaka E., Frangioni J.V., Bawendi M.G. (2006). Size series of small indium arsenide-zinc selenide core-shell nanocrystals and their application to in vivo imaging. J Am Chem Soc.
8 Pinaud F., Michalet X., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Iyer G., Weiss S. (2006). Advances in fluorescence imaging with quantum dot bio-probes. Biomaterials.
9 Koyama Y., Talanov V.S., Bernardo M., Hama Y., Regino C.A., Brechbiel M.W., Choyke P.L., Kobayashi H. (2007). A dendrimer-based nanosized contrast agent dual-labeled for magnetic resonance and optical fluorescence imaging to localize the sentinel lymph node in mice. J Magn Reson Imaging.
10 Talanov V.S., Regino C.A., Kobayashi H., Bernardo M., Choyke P.L., Brechbiel M.W. (2006). Dendrimer-based nanoprobe for dual modality magnetic resonance and fluorescence imaging. Nano Lett.